# ^99m^Tc-Labeled S-benzoylmercaptoacetyl triglycine D-galactose

Chemical name: | ^99m^Tc-Labeled S-benzoylmercaptoacetyl triglycine D-galactose
Abbreviated name: | [^99m^Tc]SBz-MAG_3_-Ga
Synonym: | [^99m^Tc]MAG_3_-Ga
Agent Category: | Compound
Target: | Lectins
Target Category: | Proteins
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure of [^99m^Tc]SBz-MAG_3_-Ga. Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=lectins&cmd=DetailsSearch)]

Lectins are proteins that bind carbohydrates reversibly and are present on the membrane surface of all prokaryotic and eukaryotic cells. It is known that the carbohydrate–lectin interactions result in the initiation of a fight against or the development of a variety of conditions such as cancer metastases (1), pathological inflammation (2), and microbial infections (3). Several clinical trials (http://clinicaltrials.gov/ct2/results?term=lectins) approved by the United States Food and Drug Administration are under way to evaluate the use of lectins to treat a variety of infections and cancerous tumors. Because of their role in the modulation of diverse physiological processes and diseases, investigators are increasingly interested in studying lectins for the development (4) and delivery of therapeutic drugs in humans (5). Although lectin glycoarrays have been used to profile different glycoproteins (6), no agents are presently available to investigate the function of the lectin-carbohydrate complexes under in vivo conditions. In an effort to develop imaging agents for the in vivo study of lectins, de Barros et al. (7) synthesized glucose (Gl), N-acetylglucosamine (NG), and galactose (Ga) respectively conjugated to S-benzoylmercaptoacetyl triglycine (SBz-MAG_3_) and labeled these compounds with ^99m^Tc to obtain [^99m^Tc]SBz-MAG_3_-Ga (or [^99m^Tc]MAG_3_-Ga), [^99m^Tc]SBz-MAG_3_-Gl (or [^99m^Tc]MAG_3_-Gl), and [^99m^Tc]SBz-MAG_3_-NG (or [^99m^Tc]MAG_3_-NG). The biodistribution of these radiolabeled carbohydrates was then studied in normal Swiss mice (7). This chapter describes the results obtained with [^99m^Tc]SBz-MAG_3_-Ga. Results obtained with [^99m^Tc]SBzMAG_3_-Gl (8) and [^99m^Tc]SBzMAG_3_-NG (9) are presented in separate chapters in MICAD (www.micad.nih.gov).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S%20benzoylmercaptoacetyl%20triglycine%20D%20glucose%20synthesis&cmd=DetailsSearch)]

The synthesis of [^99m^Tc]SBzMAG_3_-Ga was described by de Barros et al. (7). The radiochemical purity of the tracer was reported to be >90%. The radiochemical yield, specific activity, and stability of [^99m^Tc]SBzMAG_3_-Ga were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S%20benzoylmercaptoacetyl%20triglycine%20D%20glucose%20in%20Vitro%20studies&cmd=DetailsSearch)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S%20benzoylmercaptoacetyl%20triglycine%20D%20glucose%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]SBzMAG_3_-Ga was studied in normal Swiss mice (7). The animals (n = 5 mice per time point) were injected with the radiochemical, and the mice were euthanized at various time points from 5 to 60 min post-injection (p.i.) to collect all major organs and to determine the accumulated radioactivity. At 5 min p.i., maximum accumulation of label was in the bladder (44.86 ± 6.98% injected dose per gram tissue (% ID/g)), followed by the liver (11.99 ± 1.00% ID/g), kidneys (9.11 ± 2.17% ID/g), blood (4.12 ± 0.67% ID/g), and lungs (2.11 ± 0.20% ID/g). At 60 min p.i., the bladder had the highest amount of radioactivity (86.37 ± 5.06% ID/g), followed by liver (6.95 ± 0.64% ID/g), kidneys (2.47 ± 0.38% ID/g), lungs (0.91 ± 0.08% ID/g), and blood (0.86 ± 0.07% ID/g). This study indicated that radioactivity either as [^99m^Tc]SBzMAG_3_-Ga or a metabolite was excreted primarily through the urinary route. The radioactivity uptake pattern with [^99m^Tc]SBzMAG_3_-Ga was similar to that observed with [^99m^Tc]SBzMAG_3_-Gl (8) and [^99m^Tc]SBzMAG_3_-NG (9). However, accumulation of [^99m^Tc]SBz-MAG_3_-Ga was significantly (P < 0.05) higher in the liver at both 5 min and 60 min p.i. than accumulation of either [^99m^Tc]SBzMAG_3_-Gl (8.77 ± 1.22% ID/g at 5 min and 1.82 ± 0.15% ID/g at 60 min p.i.) or [^99m^Tc]SBzMAG_3_-NG (9.58 ± 0.81% ID/g at 5 min and 1.88 ± 0.44% ID/g at 60 min p.i.).

In another study, [^99m^Tc]SBzMAG_3_-Ga was injected into normal mice in the presence of 10-fold excess unlabeled Ga, and the animals were euthanized (n = 5 mice per time point) as before to determine the amount of radioactivity accumulated in the various organs (7). The biodistribution pattern of the label in the various organs was essentially as described above, but a lower amount of radioactivity was observed to accumulate in the liver, kidney, and blood (2.43 ± 0.13, 1.88 ± 0.16, and 0.53 ± 0.03% ID/g, respectively) at 60 min p.i.

From these studies, the investigators concluded that [^99m^Tc]SBzMAG_3_-Gl was selectively taken up by the liver and appeared to be a suitable for the imaging of this organ to evaluate hepatic function in rodents (7).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S-benzoylmercaptoacetyl%20triglycine%20glucose%20non%20primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S-benzoylmercaptoacetyl%20triglycine%20glucose%20non%20human%20primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S-benzoylmercaptoacetyl%20triglycine%20glucose%20human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Makrilia N., Kollias A., Manolopoulos L., Syrigos K. (2009). Cell adhesion molecules: role and clinical significance in cancer. Cancer Invest.
2 Yang R.Y., Rabinovich G.A., Liu F.T. (2008). Galectins: structure, function and therapeutic potential. Expert Rev Mol Med.
3 Haagsman H.P., Hogenkamp A., van Eijk M., Veldhuizen E.J. (2008). Surfactant collectins and innate immunity. Neonatology.
4 Ernst B., Magnani J.L. (2009). From carbohydrate leads to glycomimetic drugs. Nat Rev Drug Discov.
5 Darbre T., Reymond J.L. (2008). Glycopeptide dendrimers for biomedical applications. Curr Top Med Chem.
6 Zhao J., Patwa T.H., Qiu W., Shedden K., Hinderer R., Misek D.E., Anderson M.A., Simeone D.M., Lubman D.M. (2007). Glycoprotein microarrays with multi-lectin detection: unique lectin binding patterns as a tool for classifying normal, chronic pancreatitis and pancreatic cancer sera. J Proteome Res.
7 de Barros A.L., Cardoso V.N., Mota L.D., Alves R.J. (2010). Synthesis and biodistribution studies of carbohydrate derivatives radiolabeled with technetium-99m. Bioorg Med Chem Lett.
8 Chopra, A., 99mTc-Labeled S-benzoylmercaptoacetyl triglycine D-glucose. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Chopra, A., 99mTc-Labeled S-benzoylmercaptoacetyl triglycine N-acetylglucoseamine. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.